# ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid- D-Glu-Glu-Glu-Glu-Glu-Glu-Ala-Tyr-Gly-Trp-Met-Asp-Phe-NH_2_

Chemical name: | ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-D-Glu-Glu-Glu-Glu-Glu-Glu-Ala-Tyr-Gly-Trp-Met-Asp-Phe-NH_2_
Abbreviated name: | ^111^In-DOTA-minigastrin (MG0)
Synonym:
Agent Category: | Peptide
Target: | Gastrin/cholecystokinin-2 (CCK-2) receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=417029), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=33356159) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=887&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about.the CCK2 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+gastrin+analogs)]

The gastrointestinal peptides gastrin and cholecystokinin-2 (CCK2) have various regulatory functions in the brain and gastrointestinal tract (1). Gastrin and CCK2 have the same COOH-terminal pentapeptide amide sequence GWMDF-NH_2_, which is the biologically active site (2). Human gastrin is a peptide composed of 33 amino acids and also exists in several C-terminal–truncated forms (3). One of these truncated forms is minigastrin (MG0), which is a 13-residue peptide with the sequence of D-Glu-Glu-Glu-Glu-Glu-Glu-Ala-Tyr-Gly-Trp-Met-Asp-Phe-NH_2_. CCKs exist as a variety of biologically active molecular fragments ranging from 4 to 18 amino acids and include sulphated and unsulphated CCK8, which is an octapeptide (DYMGWMDF-NH_2_) (4). Two CCK receptor subtypes have been identified in normal tissues by their binding affinities: CCK1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK2 (CCK-B, brain) receptors have high affinity for gastrin (4). The sulphated CCK8 (sCCK8) peptide displays high affinity for both CCK1 and CCK2 receptors (CCK2R), which are G-protein–coupled receptors that have been found to be overexpressed in a variety of tumor types (5). CCK2Rs have been found most frequently in medullary thyroid carcinomas, small-cell lung cancers, astrocytomas, and stromal ovarian cancers (1). CCK1 receptors have been identified in gastroenteropancreatic tumors, meningiomas, and neuroblastomas. Radiolabeled CCK8 peptides have been studied in tumors expressing CCK2Rs with good specificity for potential in vivo imaging.

Hellmich et al. (6) discovered CCK2i4svR (a splice variant version of the CCK2R) is constitutively expressed in human colorectal and pancreatic cancers (7, 8). MG0 was N-terminally conjugated with tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid (DOTA) for radiolabeling with ^111^InCl_3_ to form ^111^In-DOTA-MG0 for imaging tumors expressing CCK2R and CCK2i4svR (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+minigastrin)]

MG0 was prepared by solid-phase peptide synthesis (9). The N-terminus was conjugated with a DOTA chelating group to produce DOTA-MG0 from N-hydroxysuccinimidyl-DOTA. DOTA-sCCK8 was purified with reverse-phase high-performance liquid chromatography. Radiolabeling was performed by mixing ^111^InCl_3_ in ammonium acetate with DOTA-MG0 and heating the mixture at 80ºC for 30 min. The radiochemical purity and specific activity were 98% and 12 TBq/mmol (324 Ci/mmol), respectively. The labeling yield was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+minigastrin+and+in+vitro)]

An in vitro receptor-binding assay of ^111^In-DOTA-MG0 was performed on HEK293 cells transfected with CCK2R (HEK293-CCK2R) and CCK2i4svR (HEK293-CCK2i4svR) (9). Binding of ^111^In-DOTA-MG0 to CCK2R and CCK2i4svR was found to be 31.5 ± 1.6% and 24.4 ± 0.1% incubation dose at 60 min of incubation at room temperature, respectively. Receptor binding in the presence of excess MG0 binding was 3.1 ± 0.4 and 2.4 ± 1.0% incubation doses, respectively. Binding to non-transfected control HEK293 cells was negligible for ^111^In-DOTA-MG0 (<0.7% incubation dose). The inhibition constant (K_i_) values of DOTA-MG0 were 128 nM for CCK2R and 10.4 nM for CCK2i4svR.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+minigastrin+and+rodentia)]

Laverman et al. (9) performed biodistribution studies of ^111^In-DOTA-MG0 in nude mice bearing a HEK293-CCK2i4svR tumor. Each mouse received 370 kBq (10 nCi) of ^111^In-DOTA-MG0 by i.v. injection. The tumor radioactivity levels (n = 4) were 6.09 ± 0.65% injected dose per gram (ID/g) at 2 h and 3.01 ± 0.67% ID/g at 24 h. The uptake in the tumor was blocked by excess MG0 to <1% ID/g at the two time points. Kidney radioactivity levels (60.2% ID/g at 2 h and 32.4% ID/g at 24 h) were significantly blocked by MG0 with 30% inhibition (P < 0.01). The radioactivity levels in the blood, lung, intestines, pancreas, spleen, and liver were <0.8% ID/g at 2 and 24 h; the liver and stomach radioactivity levels were ~1.2% ID/g at 2 and 24 h. The accumulation in the stomach was almost completely blocked by MG0, whereas little blocking was observed in the liver. The tumor/blood ratio reached 89 at 24 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+minigastrin+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+minigastrin+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+minigastrin+and+human)]

No publication is currently available.

## References

1 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
2 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
3 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for Peptide receptor-targeted radionuclide therapy. J Nucl Med.
4 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
5 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
6 Hellmich M.R., Rui X.L., Hellmich H.L., Fleming R.Y., Evers B.M., Townsend C.M. (2000). Human colorectal cancers express a constitutively active cholecystokinin-B/gastrin receptor that stimulates cell growth. J Biol Chem.
7 Smith J.P., Stock E.A., Wotring M.G., McLaughlin P.J., Zagon I.S. (1996). Characterization of the CCK-B/gastrin-like receptor in human colon cancer. Am J Physiol.
8 Smith J.P., Verderame M.F., McLaughlin P., Martenis M., Ballard E., Zagon I.S. (2002). Characterization of the CCK-C (cancer) receptor in human pancreatic cancer. Int J Mol Med.
9 Laverman P., Roosenburg S., Gotthardt M., Park J., Oyen W.J., de Jong M., Hellmich M.R., Rutjes F.P., van Delft F.L., Boerman O.C. (2008). Targeting of a CCK(2) receptor splice variant with (111)In-labelled cholecystokinin-8 (CCK8) and (111)In-labelled minigastrin. Eur J Nucl Med Mol Imaging.